# ^99m^Tc-Labeled lexatumumab

Chemical name: | ^99m^Tc-Labeled lexatumumab
Abbreviated name: | ^99m^Tc-EC-HGS-ETR2
Synonym:
Agent Category: | Antibody
Target: | Tumor necrosis factor–related apoptosis-inducing ligand receptor 2 (TRAIL-R2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the nucleotice, protein and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=8743&log$=databasead&logdbfrom=protein#refseq) information regarding TRAIL receptors.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1)]

Although anti-growth factor antibodies (Abs) are available for the treatment of cancers (1-3), another technique under investigation to treat this disease is the use of tumor necrosis factor–related apoptosis-inducing ligand (TRAIL) receptor (TRAIL-R) agonist Abs such as mapatumumab and lexatumumab (4, 5). These antibodies (Abs) activate a complex apoptotic pathway in the tumor cell, thereby inducing cell death. The apoptotic pathway and the four TRAIL-R types in humans (designated 1 through 4) have been described in detail by Johnstone et al. (4) and Ashkenazi (5). Lexatumumab (TRM-2 or HGS-ETR2) is a TRAIL-R2 monoclonal antibody (mAb) that targets TRAIL-R2; it is under commercial development and has been approved for clinical trials (http://clinicaltrials.gov/ct2/results?term=lexatumumab) by the United States Food and Drug Administration (USFDA) to treat various cancers. A similar mAb, mapatumumab (TRM-1 or HGS-ETR1), is a TRAIL-R1 mAb that acts as an agonist specifically for the TRAIL-R1 and has been approved by the USFDA for clinical trials (http://clinicaltrials.gov/ct2/results?term=Mapatumumab).

Paclitaxel and docetaxel are anti-cancer drugs that inhibit the mitosis and proliferation of cells by interfering with the depolymerization of microtubules. The mechanism of action of these drugs was discussed in detail by Saloustros et al. (6). Gong et al. observed that the anti-tumor activity of HGS-ETR2 could be enhanced in mice bearing colorectal cancer cell xenograft tumors with pretreatment with paclitaxel (7). Using HGS-ETR2 labeled with radioactive technetium (^99m^Tc) (^99m^Tc-EC-HGS-ETR2), the investigators determined that the activity of HGS-ETR2 was increased because the pretreatment with paclitaxel upregulated the expression of TRAIL-R2 in Colo205 cell xenograft tumors in nude mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of ^99m^Tc-EC-HGS-ETR2 was described by Gong et. al. (7). Briefly, ethylenedicysteine (EC) was coupled to HGS-ETR2 for the chelation of ^99m^Tc using sulfo-N-hydroxysuccinimide (NHS) and 1-ethyl-3-(3-dimethylaminopropyl)carbodiimide hydrochloride (EDC) as the coupling agents. To do this, EC, NHS, and EDC were mixed with HGS-ETR1 and incubated for 17 h at room temperature. The product, EC-HGS-ETR2, was dialyzed (buffer not described) to remove any unbound reagents. The purification and yield of EC-HGS-ETR2 were not described by the investigators. Labeling of EC-HGS-ETR1, to obtain ^99m^Tc-EC-HGS-ETR1, was performed by adding sodium pertechnetate (^99m^TcO_4_^-^) to a solution of EC-mAb in the presence of tin chloride. The number of EC per HGS-ETR2, the purification, and the yield of the radiolabeled product were not reported. Although the radiochemical purity of ^99m^Tc-EC-HGS-ETR2 was reported to be >95% (determined with radio thin-layer chromatography), the specific activity of the labeled mAb was not reported.

For use as controls during scintigraphic imaging, ^99m^Tc-EC-bovine serum albumin (BSA) and ^99m^Tc-EC-isotype control mAb were also generated as described above (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+in+vitro)]

The steady state levels of TRAIL-R1 and TRAIL-R2 were determined in Colo205 (a human colorectal cancer tumor cell line) and PA-1 (a human ovarian cancer cell line) cells using immunoblots and fluorescence-activated cell sorting (FACS) (7). Both receptor types were expressed in the two cell lines as determined with the immunoblots, but the levels were reported to be higher in the Colo205 cells than in the PA-1 cells. Similar results were obtained with FACS analysis of the two cell lines.

The concentration for 50% inhibition of cell proliferation (IC_50_) for Colo205 cells was determined to be 800 ng/mL and 150 ng/mL for HGS-ETR1 and HGS-ETR2, respectively (7). The PA-1 cells were reported to be resistant to inhibition by both the Abs even at a concentration of 800 ng/mL. This indicated that the number of TRAIL-R1 and -R2 on the PA-1 cell surface was too low to initiate apoptosis on binding of the two respective agonist TRAIL-R mAbs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+rodentia)]

Gong et al. studied the tumor uptake of ^99m^Tc-EC-HGS-ETR2 in nude mice bearing Colo205 xenograft tumors (7). Imaging studies were performed 12 days after inoculation with the cells when the tumor diameter was ~1 cm. The animals (4 or 5 mice/group) were intravenously (IV) injected with either ^99m^Tc-EC-HGS-ETR2, ^99m^Tc-EC-BSA, or the ^99m^Tc-EC-isotype control mAb, and scintigraphic images were obtained 2, 24, and 48 h later. Using computer-outlined regions of interest, the counts per pixel of the tumor site and the normal muscle were used to obtain the tumor/muscle count density ratios (TM ratio). At 2 h after administration of the radiochemicals, little difference in the TM ratios was noted between the controls and the ^99m^Tc-EC-HGS-ETR2–treated animals. However, at 24 and 48 h after the injection of radioactivity, the TM ratios for the ^99m^Tc-EC-HGS-ETR2 and the labeled control-injected animals were reported to be ~3.5–4.5 and ~2, respectively.

In another study, the Colo205 cell xenograft tumor–bearing animals (n = 3 mice) were imaged before and after (at 2 and 24 h after an IV injection of ^99m^Tc-EC-HGS-ETR2) treatment with paclitaxel (7). Animals treated with paclitaxel were imaged 24 h after administration of the drug. When imaging was performed at 2 h after treatment with the labeled mAb, little difference in the TM ratio (~2) was noted in the tumors with or without the paclitaxel treatment. By 24 h the TM ratio was reported to have increased to ~5.2 in tumors of mice treated with paclitaxel compared with a TM ratio of ~2–2.5 in the untreated mice. In the same study, PA-1 cell xenograft tumors in animals (n = 3 mice) showed little change in the TM ratio (~1.5) both at 2 and 24 h after the ^99m^Tc-EC-HGS-ETR2 injection. This indicated that very little of the labeled mAb bound to the tumors derived from the PA-1 cells. No blocking studies to demonstrate specific binding were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Chase J.L. (2008). Clinical use of anti-vascular endothelial growth factor monoclonal antibodies in metastatic colorectal cancer. Pharmacotherapy.
2 Patel D.K. (2008). Clinical use of anti-epidermal growth factor receptor monoclonal antibodies in metastatic colorectal cancer. Pharmacotherapy.
3 Sachdev D., Singh R., Fujita-Yamaguchi Y., Yee D. (2006). Down-regulation of insulin receptor by antibodies against the type I insulin-like growth factor receptor: implications for anti-insulin-like growth factor therapy in breast cancer. Cancer Res.
4 Johnstone R.W., Frew A.J., Smyth M.J. (2008). The TRAIL apoptotic pathway in cancer onset, progression and therapy. Nat Rev Cancer.
5 Ashkenazi A. (2008). Directing cancer cells to self-destruct with pro-apoptotic receptor agonists. Nat Rev Drug Discov.
6 Saloustros E., Mavroudis D., Georgoulias V. (2008). Paclitaxel and docetaxel in the treatment of breast cancer. Expert Opin Pharmacother.
7 Gong J., Yang D., Kohanim S., Humphreys R., Broemeling L., Kurzrock R. (2006). Novel in vivo imaging shows up-regulation of death receptors by paclitaxel and correlates with enhanced antitumor effects of receptor agonist antibodies. Mol Cancer Ther.